# 4-[^76^Br]Bromophenyl-1,4-diazabicyclo(3.2.2) nonane-4-carboxylate

Chemical name: | 4-[^76^Br]Bromophenyl-1,4-diazabicyclo(3.2.2) nonane-4-carboxylate
Abbreviated name: | [^76^Br]SSR180711
Synonym:
Agent category: | Compound
Target: | Neuronal α7 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^76^Br
Activation: | No
Studies: | - In vitro; - Other Non-primate Mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380, which has been developed as a single-photon emission computed tomography agent for the non-invasive study of α4β2 nAChR in the brain. There are some implications that α7 nAChRs may play a role in the pathophysiology of neuropsychiatric disorders (6-8); however, there have been no clinical studies of α7 nAChRs using PET ligands. 4-Bromophenyl-1,4-diazabicyclo(3.2.2) nonane-4-carboxylate (SSR180711) has been shown to be a potent and selective partial agonist for α7 nAChRs with nanomolar affinity (9). [^76^Br]SSR180711 is being developed as a PET agent for the non-invasive study of α7 nAChR in the brain (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20synthesis)]

Hashimoto et al. (10) reported the synthesis of [^76^Br]SSR180711 by bromination of 4-(tributylstannyl)phenyl 2,5-diazabicyclo[3.2.2] nonane-2-carboxylate in the presence of chloramine-T and [^76^Br]bromide in an ethanol solution. The mixture was heated for 30 min at 75°C. Average radiochemical yield was 16.7 ± 6.14% at the end of synthesis. The radiochemical purity was >99% with a specific activity of 8.11 ± 1.65 GBq/µmol (219 ± 45 mCi/µmol; n = 9) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20in%20vitro)]

Biton et al. (9) reported that SSR180711 exhibited inhibition constant (K_i_) values (obtained with the use of [^3^H]α-bungarotoxin) of 22 ± 4 and 14 ± 1 nM in rat and human α7 nAChRs, respectively. On the other hand, SSR180711 exhibited little affinity for α4β2, α2β4, and α3β4 nAChRs as well as other receptors tested.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20(primate%20not%20human))]

[^76^Br]SSR180711 PET studies with monkeys (n = 3) showed substantial brain accumulation with selective maximal uptake in the regions of the hippocampus, cortex and basal ganglia (0.010-0.013%dose/cc) 30–40 min after injection with gradual washouts (10); the cerebellum (0.009%dose/cc) showed lower binding than the other brain regions. [^76^Br]SSR180711 radioactivity level in the brain regions was reduced to the background level of the cerebellum by pretreatment with the α7 nAChR agonist SSR180711 (5.0 mg/kg, 30 min). However, the accumulation of radioactivity in the brain regions after intravenous administration of [^76^Br]SSR180711 was not affected by pretreatment with the selective α4β2 nAChR agonist A-85380 (1.0 mg/kg, 30 min).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SSR180711%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Gotti C., Zoli M., Clementi F. (2006). Brain nicotinic acetylcholine receptors: native subtypes and their relevance. Trends Pharmacol Sci.
7 Nomikos G.G., Schilstrom B., Hildebrand B.E., Panagis G., Grenhoff J., Svensson T.H. (2000). Role of alpha7 nicotinic receptors in nicotine dependence and implications for psychiatric illness. Behav Brain Res.
8 Nordberg A. (2001). Nicotinic receptor abnormalities of Alzheimer's disease: therapeutic implications. Biol Psychiatry.
9 Biton B., Bergis O.E., Galli F., Nedelec A., Lochead A.W., Jegham S., Godet D., Lanneau C., Santamaria R., Chesney F., Leonardon J., Granger P., Debono M.W., Bohme G.A., Sgard F., Besnard F., Graham D., Coste A., Oblin A., Curet O., Vige X., Voltz C., Rouquier L., Souilhac J., Santucci V., Gueudet C., Francon D., Steinberg R., Griebel G., Oury-Donat F., George P., Avenet P., Scatton B. (2007). SSR180711, a novel selective alpha7 nicotinic receptor partial agonist: (1) binding and functional profile. Neuropsychopharmacology.
10 Hashimoto K., Nishiyama S., Ohba H., Matsuo M., Kobashi T., Takahagi M., Iyo M., Kitashoji T., Tsukada H. (2008). [11C]CHIBA-1001 as a novel PET ligand for alpha7 nicotinic receptors in the brain: a PET study in conscious monkeys. PLoS ONE.